# Hyperpolarized α-keto[1-^13^C]isocaproate as a ^13^C magnetic resonance spectroscopic agent for profiling branched chain amino acid metabolism in tumors

Chemical name: | Hyperpolarized α-keto[1-^13^C]isocaproate | [image]
Abbreviated name: | [1-^13^C]KIC | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | Branched chain amino acid transferase (BCAT) | [image]
Target Category: | Enzymes | [image]
Method of detection: | Magnetic resonance imaging (MRI)/magnetic resonance spectroscopy (MRS) | [image]
Source of signal / contrast: | Hyperpolarized ^13^C | [image]
Activation: | Yes | [image]
Studies: | - In vitro; - Rodents | Click on the PubChem for additional information of [1-^13^C]KIC (http://pubchem.ncbi.nlm.nih.gov/summary/summary.cgi?cid=44552616&loc=ec_rcs) and [1-^13^C]leucine (http://pubchem.ncbi.nlm.nih.gov/summary/summary.cgi?cid=44552618&loc=ec_rcs).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Magnetic+resonance+spectroscopy)]

Magnetic resonance spectroscopy (MRS) is a technique that allows us to non-invasively detect multiple small metabolites within cells or extracellular spaces in vivo (1, 2). The clinical use of MRS as an adjunct to magnetic resonance imaging (MRI), particularly in cancer detection and treatment response evaluation, has expanded dramatically over the past several years. Although MRS is theoretically applicable to any nucleus possessing spin, the most important and more frequently investigated applications are in proton (^1^H) and carbon-13 (^13^C) (1, 3, 4). ^13^C MRS is superior to ^1^H MRS in many respects (5-7). ^13^C MRS can provide specific information about the identity and structure of biologically important compounds. The chemical shift range for carbon (~250 ppm) is much larger than that for proton (~15 ppm), allowing for improved resolution of metabolites. In addition, the T_1_ relaxation time of ^13^C in small molecules is much longer than that of ^1^H (0.1–2.0 s in a magnetic field of 0.1–3.0 T), allowing the generation of hyperpolarized ^13^C-labeled tracers outside the subject and the MRI scanner. Some of these tracers are endogenous and therefore have lower toxicity than drugs and exogenous contrast media (2). However, ^13^C MRS is limited by the low natural abundance of ^13^C (1.1%) and its low magnetogyric ratio (γ of ^13^C is one quarter that of ^1^H) (1, 6).

Several techniques have been used to overcome the ^13^C MRS limitation through enhancing the polarization of nuclear spins. One technique is proton decoupling, which eliminates the coupling of ^1^H with ^13^C by irradiating the entire ^1^H resonance absorption range and consequently collapsing ^13^C resonances to singlets (8, 9). The signal/noise ratio of ^13^C resonances has been shown to be significantly increased with proton decoupling. Another technique is known as dynamic nuclear polarization (DNP), which introduces one or more ^13^C molecules into a metabolic substrate (3, 10, 11). DNP transfers high electron spin polarization to nuclear spins via microwave irradiation. Nearly 100% nuclear polarization for ^1^H and 50% for ^13^C can be achieved in various organic molecules when DNP is performed in a strong magnetic field and at cryogenic temperatures. Hyperpolarization of protons ex vivo is less interesting for medical applications, because most of the hyperpolarization would have vanished before the molecule reaches the target organ. However, the T_1_ of ^13^C in small molecules, in general, is much longer than the T_1_ of protons. A large number of low molecular weight substances with ^13^C T_1_ in excess of 10 s are available. Replacing the ^12^C isotope (98.9% natural abundance) with the ^13^C isotope at a specific carbon or carbons in a metabolic substrate does not affect the substrate's biochemistry. With ^13^C MRS, the body tissues are virtually invisible, and only regions where the hyperpolarized ^13^C-labeled substance is present will appear in the generated images. Thus, ^13^C-labeled substrates can provide >10,000-fold enhancement of the ^13^C MRS signals from the substrate and its subsequent metabolic products, allowing the assessment of changes in metabolic fluxes in vivo through glycolysis, citric acid cycle, and fatty acid synthesis (2, 11, 12). Vascular and perfusion imaging can also be performed without background signal from surrounding tissues (6, 13).

Karlsson et al. generated a hyperpolarized small molecule, α-keto[1-^13^C]isocaproate ([1-^13^C]KIC) as a ^13^C MRS agent for imaging the molecular signature of branched chain amino acid metabolism, which is regulated by the branched chain amino acid transferase (BCAT) (5). There are two isoforms, BCAT1 and BCAT2, that code for mitochondrial and cytosolic BCAT, respectively (5, 14). BCAT is highly expressed in early embryogenesis, and it is also a target for MYC activity during oncogenesis. BCAT has been shown to be a useful marker for grading and genetic characterization of tumors. KIC is a substrate of BCAT and is metabolized to leucine in vivo. Karlsson et al. demonstrated that metabolism of the hyperpolarized [1-^13^C]KIC yielded unprecedented MRI contrast between EL4 murine lymphoma and surrounding healthy tissue, but yielded no contrast between R3230AC rat mammary adenocarcinoma and its surrounding tissue. The [1-^13^C]leucine signal detected in the two tumor models correlated well with ex vivo measurements of the BCAT activity in the two tumor tissues. The investigators concluded that the understanding of metabolic differences between tumors could be advanced with use of the hyperpolarized [1-^13^C]KIC biomarker in assessing tissue BCAT activity in vivo by means of the [1-^13^C]leucine signal (5).

### Related Resource Links:

- Chapters of ^13^C MRS in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=13C%2C+MRI+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- BCAT articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=BCAT)
- Gene information of BCAT (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=search&Term=((BCAT)%20AND%20%22Homo%20sapiens%22%5bporgn:__txid9606%5d)%20AND%20alive%5bprop%5d%20NOT%20newentry%5bgene%5d&log$=databasead1&logdbfrom=protein)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=imaging+and+branched+amino+acid+metabolism+ketoisocaproate)]

Karlsson et al. detailed the generation of hyperpolarized [1-^13^C]KIC (5). The starting agent [1-^13^C]KIC, as a sodium salt, was commercially available. [1-^13^C]KIC was first converted to the acid form by acidifying an aqueous solution of the salt to pH < 1 with sulfuric acid, followed by an extraction of the acidified solution with diethylether. After drying the ether phase with anhydrous magnesium sulfate, the solvent was removed in vacuum. The DNP preparation of [1-^13^C]KIC was established by dissolving the trityl radical OX063 (tris(8-carboxyl-2,2,6,6-tetra(2-(1hydroxyethyl))-benzo[1,2-d:4,5-d’]bis(1,3)dithiole-4-yl)methyl sodium) in the acid, followed by adding trimeric gadolinium 2-[4,7,10-tris(carboxymethyl)-1,4,7,10-tetraazacyclododec-1-yl] acetic acid (Gd-DOTA) complex. Addition of the Gd-DOTA complex could enhance the solid state polarization, and the negative effect on the relaxation time constant of the hyperpolarized substance in solution was negligible at the concentrations used. This DNP preparation of [1-^13^C]KIC was hyperpolarized in a polarizer, and the hyperpolarized sample was subsequently dissolved in an aqueous solution of sodium hydroxide and phosphate buffer (40 mmol; osmolality was adjusted with NaCl to 210 mOsm) to provide a 20-mmol solution of hyperpolarized [1-^13^C]KIC at pH 7.4 ± 0.1, an osmolality of 290 ± 10 mOsm, T_1_ (9.4 T) of 55 ± 3 s, and a polarization of 32 ± 3% at the time of administration. A dose of 0.175 mmol/kg was infused into animals within 6 s. MRS was started at 20 s after start of the infusion. The total acquisition time was 12 s. A 30% polarization is equal to a signal enhancement on the order of 10^5^ relative to the equilibrium ^13^C spin polarization in the medical scanner of a 3-T magnetic field at 310 K (~0.0003%) (5).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=imaging+and+branched+amino+acid+metabolism+ketoisocaproate)]

Karlsson et al. measured the BCAT activity in cell cultures of EL4 and R3230AC lines with spectrophotometric assay (5). Significantly high BCAT activity was observed in EL4 (16.6 ± 1.7 U/g protein) as compared with R3230AC cell suspensions (3.7 ± 1.8 U/g protein), which is in agreement with the data from in vivo [1-^13^C]KIC MRS and spectrophotometric assays of ex vivo tumor tissues (see below).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=imaging+and+branched+amino+acid+metabolism+ketoisocaproate)]

Karlsson et al. first assessed the BCAT reaction with [1-^13^C]KIC in mice bearing EL4 tumors (n = 5) (5). Upon [1-^13^C]KIC injection, ample ^13^C signal was detectable in mouse tissues within a few seconds, both for [1-^13^C]KIC (δ^13^C = 172.6 ppm) and its transamination product [1-^13^C]leucine (δ^13^C = 176.8 ppm). With the exception of [1-^13^C]leucine, no other reaction product was quickly detectable. In EL4 tumor, the maximum [1-^13^C]leucine signal was detected at ~20 s after injection of [1-^13^C]KIC. The signal/noise ratio of [1-^13^C]leucine was 13.3 ± 6.3 (mean ± SD) in tumor. The [1-^13^C]leucine signal was 6.9 ± 1.0 times higher in tumor than the highest [1-^13^C]leucine signal in surrounding tissues. Overlay of the ^13^C chemical shift images with the anatomical ^1^H images showed that [1-^13^C]KIC migrated to the gastrointestinal tract and tumor within the first 20 s after injection. Both [1-^13^C]KIC and [1-^13^C]leucine signals lost the vast majority of their enhanced ^13^C spin polarization after ~100 s.

To evaluate the influence of [1-^13^C]KIC uptake on the contrast of [1-^13^C]leucine signal between tumor and surrounding tissue, Karlsson et al. analyzed the KIC levels in tissues ex vivo with an optical test. Total KIC pools before injection were 0.05 ± 0.05 and 0.17 ± 0.05 µmol per gram tissue (µmol/g) for tumor and muscle, respectively, while at 25 s after injection these values increased to 0.67 ± 0.04 and 0.61 ± 0.05 µmol/g (n = 5 for all groups) for tumor and muscle, respectively. Muscle was chosen for comparison with tumor because it was among the tissues with the highest BCAT activity in healthy mammals and thus was a determinant of the tissue contrast of branched chain amino acid metabolism between tumor and healthy tissue. Because BCAT has a low Michaelis constant (K_M_ = 0.14 mmol/l) for KIC, levels of the substrate after injection of hyperpolarized [1-^13^C]KIC did not limit the BCAT catalyzed reaction either in tumor or muscle tissue, and substrate availability was not expected to contribute significantly to tissue contrast of branched chain amino acid metabolism between tumor and surrounding tissue.

To assess tumor-specific differences in branched chain amino acid metabolism, Karlsson et al. also performed imaging experiments in a rat R3230AC breast cancer model (5). As for the EL4 lymphoma model, the hyperpolarized [1-^13^C]KIC signal was evenly distributed in the rat tissues. Turnover of [1-^13^C]KIC to [1-^13^C]leucine in the tumor was, however, minor. Substantial [1-^13^C]KIC signal in the tumor indicated that [1-^13^C]leucine synthesis was not limited by low tissue perfusion, which was further confirmed with KIC measurements ex vivo. KIC uptake above the BCAT K_M_ was found both for muscle (0.07 ± 0.003 µmol/g before KIC infusion, 151 ± 14 µmol/g after KIC infusion) and tumor (0.05 ± 0.01 µmol/g before KIC infusion, 199 ± 56 µmol/g after KIC infusion). BCAT activities were comparable in rat muscle, R3230AC tumor, and mouse muscle, but were substantially increased in EL4 tumors.

Tissue perfusion in both tumor models was also evaluated with hyperpolarized [1-^13^C]pyruvate. Hyperpolarized [1-^13^C]pyruvate is a well established tumor marker because of increased levels of anaerobic glycolysis, and the resultant high lactate dehydrogenase catalyzes flux of ^13^C signal between [1-^13^C]pyruvate and [1-^13^C]lactate in neoplastic tissues. Therefore, [1-^13^C]pyruvate was used as a reference substrate both in EL4 and R3230AC tumors. The expected high [1-^13^C]lactate formation was observed in both tumor models, suggesting high tissue perfusion and efficient cellular monocarboxylic acid uptake in both models. The high [1-^13^C]lactate formation also indicated that the higher [1-^13^C]leucine formation resulted from the higher BCAT activity or co-substrate availability in EL4 tumors versus R3230AC tumors rather than from higher tissue perfusion and marker uptake. This indicates the use of hyperpolarized [1-^13^C]pyruvate as a general in vivo tumor marker, whereas hyperpolarized [1-^13^C]KIC provides a discriminative marker for the non-invasive profiling of branched chain amino acid metabolism in tumors.

Karlsson et al. concluded that [1-^13^C]KIC MRS is sufficiently sensitive for in vivo assay of BCAT activity (5). Information on the distribution and metabolism of [1-^13^C]KIC and [1-^13^C]leucine can be sensitively obtained within the first minute after injection. Hyperpolarized [1-^13^C]KIC is a biomarker that specifically reports on metabolism by BCATs in vivo in small animals (5).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Kurhanewicz J., Bok R., Nelson S.J., Vigneron D.B. (2008). Current and potential applications of clinical 13C MR spectroscopy. J Nucl Med.
2 Golman K., Ardenkjaer-Larsen J.H., Petersson J.S., Mansson S., Leunbach I. (2003). Molecular imaging with endogenous substances. Proc Natl Acad Sci U S A.
3 Hu S., Lustig M., Chen A.P., Crane J., Kerr A., Kelley D.A., Hurd R., Kurhanewicz J., Nelson S.J., Pauly J.M., Vigneron D.B. (2008). Compressed sensing for resolution enhancement of hyperpolarized 13C flyback 3D-MRSI. J Magn Reson.
4 Larson P.E., Kerr A.B., Chen A.P., Lustig M.S., Zierhut M.L., Hu S., Cunningham C.H., Pauly J.M., Kurhanewicz J., Vigneron D.B. (2008). Multiband excitation pulses for hyperpolarized 13C dynamic chemical-shift imaging. J Magn Reson.
5 Karlsson M., Jensen P.R., Zandt R.I., Gisselsson A., Hansson G., Duus J.O., Meier S., Lerche M.H. (2010). Imaging of branched chain amino acid metabolism in tumors with hyperpolarized (13)C ketoisocaproate. Int J Cancer.
6 Mansson S., Johansson E., Magnusson P., Chai C.M., Hansson G., Petersson J.S., Stahlberg F., Golman K. (2006). 13C imaging-a new diagnostic platform. Eur Radiol.
7 Golman K., Olsson L.E., Axelsson O., Mansson S., Karlsson M., Petersson J.S. (2003). Molecular imaging using hyperpolarized 13C. Br J Radiol.
8 Chen A.P., Tropp J., Hurd R.E., Van Criekinge M., Carvajal L.G., Xu D., Kurhanewicz J., Vigneron D.B. (2009). In vivo hyperpolarized 13C MR spectroscopic imaging with 1H decoupling. J Magn Reson.
9 Ardenkjaer-Larsen J.H., Fridlund B., Gram A., Hansson G., Hansson L., Lerche M.H., Servin R., Thaning M., Golman K. (2003). Increase in signal-to-noise ratio of > 10,000 times in liquid-state NMR. Proc Natl Acad Sci U S A.
10 Chen A.P., Kurhanewicz J., Bok R., Xu D., Joun D., Zhang V., Nelson S.J., Hurd R.E., Vigneron D.B. (2008). Feasibility of using hyperpolarized [1-13C]lactate as a substrate for in vivo metabolic 13C MRSI studies. Magn Reson Imaging.
11 Albers M.J., Bok R., Chen A.P., Cunningham C.H., Zierhut M.L., Zhang V.Y., Kohler S.J., Tropp J., Hurd R.E., Yen Y.F., Nelson S.J., Vigneron D.B., Kurhanewicz J. (2008). Hyperpolarized 13C lactate, pyruvate, and alanine: noninvasive biomarkers for prostate cancer detection and grading. Cancer Res.
12 Gallagher F.A., Kettunen M.I., Day S.E., Hu D.E., Ardenkjaer-Larsen J.H., Zandt R., Jensen P.R., Karlsson M., Golman K., Lerche M.H., Brindle K.M. (2008). Magnetic resonance imaging of pH in vivo using hyperpolarized 13C-labelled bicarbonate. Nature.
13 Olsson L.E., Chai C.M., Axelsson O., Karlsson M., Golman K., Petersson J.S. (2006). MR coronary angiography in pigs with intraarterial injections of a hyperpolarized 13C substance. Magn Reson Med.
14 Jensen P.R., Karlsson M., Meier S., Duus J.O., Lerche M.H. (2009). Hyperpolarized amino acids for in vivo assays of transaminase activity. Chemistry.